# ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_

Chemical name: | ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_
Abbreviated name: | ^68^Ga-DOTA-E-[c(RGDfK)]_2_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). Extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) contain a tripeptide sequence consisting of Arg-Gly-Asp (RGD), which binds to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Janssen et al. (13) reported the development of ^111^In-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_ (^111^In-DOTA-E-[c(RGDfK)]_2_) for single-photon emission computed tomography imaging α_v_β_3_ receptors in nude mice bearing ovarian carcinoma tumors. Dijkgraaf et al. (14) also reported the evaluation of ^68^Ga-DOTA-E-[c(RGDfK)]_2_ for positron emission tomography (PET) imaging α_v_β_3_ receptors in tumor, which is the topic of this chapter.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+synthesis)]

Dijkgraaf et al. (14) prepared the synthesis of ^68^Ga-DOTA-E-[c(RGDfK)]_2_ by reacting DOTA-E-[c(RGDfK)]_2_ with ^68^Ga in ammonium acetate buffer (pH ~5.5) at 95°C for 20 min. Radiochemical purity was ~98% as determined by high-performance liquid chromatography. The maximum specific activity was 11.2 MBq/nmol (0.3 mCi/nmol). ^68^Ga-DOTA-E-[c(RGDfK)]_2_ was stable in phosphate-buffered saline and human serum at 37°C for 2 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+in+vitro)]

Dijkgraaf et al. (14) performed in vitro solid-phase binding assays of ^111^In-DOTA-E-[c(RGDfK)]_2_ with human α_v_β_3_ integrin. ^nat^Ga-DOTA-E-c(RGDfK) (monomer) had an IC_50_ value of 23.9 ± 1.22 nM. ^nat^Ga-DOTA-E-[c(RGDfK)]_2_ (dimer) had an IC_50_ value of 8.99 ± 1.20 nM. ^nat^Ga-DOTA-E-{E-[c(RGDfK)]_2_}_2_ (tetramer) had an IC_50_ value of 1.74 ± 1.18 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+rodentia)]

Dijkgraaf et al. (14) performed ex vivo biodistribution studies of ^68^Ga-DOTA-E-[c(RGDfK)]_2_ in nude mice (n = 3/group) bearing SK-RC-52 human renal carcinoma tumors at 2 h after injection. The tumor accumulation was 5.2 ± 0.3% injected dose/gram (ID/g). The organ with the highest accumulation was the intestine (~5% ID/g), followed by the kidney (~4% ID/g), spleen (~3% ID/g), liver (~2% ID/g) and colon (~2% ID/g). Coinjection of 100-fold excess DOTA-E-[c(RGDfK)]_2_ resulted in >90% reduction of radioactivity in the tumor. The accumulation was also markedly reduced in the liver, lung, intestine, colon and spleen (this may be partly mediated by α_v_β_3_ integrin in these tissues) but not in the kidney. PET scan showed that the tumor was clearly visualized at 2 h after injection of 10 MBq (0.27 mCi) ^68^Ga-DOTA-E-[c(RGDfK)]_2_. Some accumulation was observed in the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga+RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Janssen M.L., Oyen W.J., Dijkgraaf I., Massuger L.F., Frielink C., Edwards D.S., Rajopadhye M., Boonstra H., Corstens F.H., Boerman O.C. (2002). Tumor targeting with radiolabeled alpha(v)beta(3) integrin binding peptides in a nude mouse model. Cancer Res.
14 Dijkgraaf I., Yim C.B., Franssen G.M., Schuit R.C., Luurtsema G., Liu S., Oyen W.J., Boerman O.C. (2011). PET imaging of alphavbeta integrin expression in tumours with Ga-labelled mono-, di- and tetrameric RGD peptides. Eur J Nucl Med Mol Imaging.